# ^99m^Tc-Hydrazinonicotinic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | ^99m^Tc-Hydrazinonicotinic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Hydrazinonicotinic acid (HYNIC) is a coupling agent for ^99m^Tc labeling of peptides that can achieve high specific activities without affecting the receptor-binding ability of the amino acid sequence. ^99m^Tc is bound to the hydrazine group, and other coordination sites can be occupied by one or more coligands. Liu et al. (13) reported the success of radiolabeling the cyclo(Arg-Gly-Asp-D-Phe-Lys) (c(RGDfK)) dimer linked by glutamic acid that was conjugated with HYNIC. Trisodium triphenylphosphine-3,3’,3’’-trisulfonate (TPPTS) and tris(hydroxymethyl)-methylglycine (tricine) as coligands. ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) showed high tumor accumulation in nude mice bearing human tumor xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+synthesis)]

Liu et al. (13) reported the synthesis of ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) by incubation of 20 μg HYNIC-E-[c(RGDyK)]_2_, 6.5 mg tricine, 5 mg TPPTS, and 1.85 GBq (50 mCi ) Na[^99m^TcO_4_] for 10 min at 100ºC. Radiochemical purity was >90% with a specific activity of ~370 GBq/μmol (10 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+in+vitro)]

Liu et al. (14) performed in vitro competition of ^99^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) with biotinylated vitronectin. ^99^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) had an IC_50_ value of 1.7 ± 0.5 nM. E-[c(RGDfK)]_2_ had an IC_50_ value of 0.6 ± 0.4 nM. The in vitro solution stability of ^99^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) was tested by incubating the radiolabeled peptide in phosphate-buffered solution that contained 1.0 mg/ml cysteine at 37ºC for up to 6 h. No significant degradation of ^99^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) was observed under these conditions. Janssen et al. (15) reported that the receptor-binding fraction of ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_(tricine)(TPPTS) for conditions representing infinite receptor concentration was >70% using cultured human ovarian carcinoma IGROV-1 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+rodentia)]

Janssen et al. (15) performed biodistribution studies of ^99m^Tc-HYNIC-E-c(RGDfK) and ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_ in nude mice bearing human OVCAR-3 ovary carcinoma tumors. Tumor uptake peaked at 5.8 ± 0.7% injected dose (ID)/g (1 h) and 5.2 ± 0.6% ID/g (30 min) for the dimer and the monomer, respectively. At 1, 2, and 4 h after injection, uptake of the dimer in the tumors was significantly higher than that of the monomer. Tumor/blood ratios were similar at all time points, the highest at 24 h with a value of 63 for both compounds. At all time points, kidney accumulation of the dimer was significantly higher than kidney accumulation of the monomer. Both peptides exhibited similar accumulation in the spleen, liver, and lung.

Liu et al. (16) performed biodistribution studies of ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_ in nude mice bearing human MDA-MB-435 breast carcinoma tumors. Tumor uptake values were 3.50% ID/g at 5 min, 3.59% ID/g at 30 min, 3.38% ID/g at 60 min, and 3.82% ID/g at 120 min. The organ with the highest uptake was the kidney (14.33% ID/g at 120 min), followed by the intestine (4.95% ID/g at 120 min), lung (2.83% ID/g at 120 min), and liver (3.11% ID/g at 120 min). Blood levels (% ID/g) were 2.70 at 5 min, 1.66 at 30 min, 1.60 at 60 min, and 0.52 at 120 min. Co-injection of E-[c(RGDfK)]_2_ (30 mg/kg) resulted in a significant reduction of radioactivity in the tumor, lung, liver, spleen, and intestine. The radioactivity in the kidney and muscle was also slightly reduced. Jia et al. (17) performed single-photon emission computed tomography imaging in nude mice bearing U87MG human glioma tumors with 14.8 MBq (0.4 mCi) of ^99m^Tc-HYNIC-E-[c(RGDfK)]_2_. The tumors were clearly visualized at 4 h after injection because of fast clearance of the tracer from the liver and lungs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+RGD+human)]

No publication is currently available.

## NIH Support

R01 CA115883-01A2

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Liu S., Edwards D.S., Ziegler M.C., Harris A.R., Hemingway S.J., Barrett J.A. (2001). 99mTc-labeling of a hydrazinonicotinamide-conjugated vitronectin receptor antagonist useful for imaging tumors. Bioconjug Chem.
14 Liu S., Hsieh W.Y., Jiang Y., Kim Y.S., Sreerama S.G., Chen X., Jia B., Wang F. (2007). Evaluation of a (99m)Tc-labeled cyclic RGD tetramer for noninvasive imaging integrin alpha(v)beta3-positive breast cancer. Bioconjug Chem.
15 Janssen M.L., Oyen W.J., Dijkgraaf I., Massuger L.F., Frielink C., Edwards D.S., Rajopadhye M., Boonstra H., Corstens F.H., Boerman O.C. (2002). Tumor targeting with radiolabeled alpha(v)beta(3) integrin binding peptides in a nude mouse model. Cancer Res.
16 Liu S., Hsieh W.Y., Kim Y.S., Mohammed S.I. (2005). Effect of coligands on biodistribution characteristics of ternary ligand 99mTc complexes of a HYNIC-conjugated cyclic RGDfK dimer. Bioconjug Chem.
17 Jia B., Shi J., Yang Z., Xu B., Liu Z., Zhao H., Liu S., Wang F. (2006). 99mTc-labeled cyclic RGDfK dimer: initial evaluation for SPECT imaging of glioma integrin alphavbeta3 expression. Bioconjug Chem.